# Bombesin peptide conjugated–cross-linked iron oxide-Cy5.5

Chemical name: | Bombesin peptide conjugated–cross-linked iron oxide-Cy5.5
Abbreviated name: | BN-CLIO-Cy5.5
Synonym: | (FITC)BCDDDGQRLGNQWAVGHLM-CLIO(Cy5.5), BN-CLIO(Cy5.5)
Agent Category: | Peptide
Target: | Gastrin-releasing peptide receptor
Target Category: | Receptor
Method of detection: | Magnetic resonance imaging (MRI), Optical (NIRF)
Source of signal: | Iron oxide, Cy5.5, FITC
Activation: | No
Studies: | - In vitro; - Rodents | Structure is not available in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=bombesin%20pancreatic%20ductal%20adenocarcinoma)]

One of the leading causes of cancer death in the United States of America is pancreatic ductal adenocarcinoma (PDAC). Late diagnosis of this tumor and its strong drug resistance are factors that lead to the low survival rate of PDAC patients (1). Limitations in diagnostic techniques and lack of specific symptoms often account for the late diagnosis of PDAC. It will be of tremendous help to patients to develop a technique for early diagnosis of PDAC.

The design of molecules or peptides that specifically target the overexpressed or upregulated receptors on cancerous cells is an important strategy in the development of therapeutic and diagnostic drugs. This strategy, however, does not work well in PDAC because many of these receptors also express in normal pancreas. An inverse strategy, targeting the receptors on normal cells instead of those on tumor cells, was thus developed by Montet et al. (1) to overcome this difficulty. It has been shown that targeting the normal cells instead of the tumor cells enhances the visualization of tumors in liver or lymph nodes by molecular resonance imaging (MRI) (2, 3).

Bombesin (BN)-like peptide is an analog of human gastrin-releasing peptide (GRP) that binds to GRP receptors (GRP-R). BN peptides educe such biological responses as: secretion of adrenal, pituitary, and gastrointestinal hormones; gastric acid secretion; modulation of neuronal firing rate; and regulation of smooth muscle contraction (4). BN-related peptide receptors can be divided into four subtypes: GRP-R (BB2, BRS-2), neuromedin B receptor (NMB-R, BB1, BRS-1), the orphan receptor bb3-R (BRS-3), and the amphibian receptor bb4-R. Several human cancers, including prostate, breast, lung, and pancreatic cancers, express receptors for BN-like peptides. The BN-like peptides have been radiolabeled with different radionuclei for in vivo imaging of various cancers (5-8). However, it was reported that BN peptide-binding receptors were present in normal pancreas but not in PDAC (9). This provides a great potential to develop the inverse strategy for detecting PDAC at an early stage. The BN binding receptor was reported to be able to internalize ligands, and consequently could provide great potential for accumulation of nanoparticles for detection (10-12). A BN receptor-targeted peptide was therefore used to conjugate with CLIO-Cy5.5, a nanoparticle that consists of a cross-linked superparamagnetic iron oxide nanoparticle (CLIO) and a near infrared (NIR) fluorochrome (Cy5.5) and thus possesses both MRI and NIR fluorescence (NIRF) imaging modalities.

BN-CLIO-Cy5.5 was prepared by conjugating the fluorescein (FITC)-labeled BN peptide (FITC-BCDDDGQRLGNQWAVGHLM) with the nanoparticle CLIO-Cy5.5. It serves as a contrast agent for MRI and, in the meantime, provides a NIRF image.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=bombesin%20nanoparticle%20conjugate)]

The synthesis of FITC-BCDDDGQRLGNQWAVGHLM-CLIO-Cy5.5 (BN-CLIO-CY5.5) and FITC-BCDDDGQMLGNHLAVGQWR (ScrBN-CLIO-Cy5.5, control peptide) was described by Montet et al. (1). In brief, the peptides were synthesized using solid-phase peptide synthesis via 9-fluorenylmethyloxycarbonyl (Fmoc) chemistry. The N-terminus beta-alanine (B) was used to conjugate with FITC and the thiol group of cysteine was utilized to conjugate the peptide with CLIO-Cy5.5 nanoparticles. CLIO-NH_2_ nanoparticles (produced by coating iron oxide nanoparticles with dextran, followed by cross-linking with epichlorohydrin, and then activated by reacting with ammonia (13, 14)) were mixed with Cy5.5 solution to produce 5.1 dyes per nanoparticle. Purified CLIO(NH_2_)-Cy5.5 was further activated by reacting with succinimidyl iodoacetate. Activated CLIO-Cy5.5 was then conjugated with a BN peptide through cysteine. The size of the nanoparticle was determined to be 35 nm using laser light scattering method, with an average of 50 peptides per iron oxide particle.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=pancreas%20bombesin%20CLIO)]

Normal mouse pancreas tissue was used to prove the binding of BN-CLIO-Cy5.5 with the BN receptor (1). The tissues were treated with BN-CLIO-Cy5.5 or ScrBN-CLIO-Cy5.5; BN-CLIO-Cy5.5 generated a darker stain than ScrBN-CLIO-Cy5.5 with a fluorescein hapten visualization method (15). The result was verified using a fluorescein hapten assay (15) to quantify the amount of fluorescein that bound to the BN receptors. There was 3.5-fold more BN-CLIO-Cy5.5 bound to the tissue specimen than ScrBN-CLIO-Cy5.5.

A tissue microarray consisting of 5 normal human pancreas specimens and 13 pancreatic ductal adenocarcinomas was used to assess the method (1). It appeared that the normal pancreas tissue showed a much darker stain than the ductal adenocarcinoma specimens. The result from mouse and human pancreas tissue showed that BN-CLIO-Cy5.5 appeared to bind to normal pancreas and not to PDAC.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=bombesin%20CLIO)]

Normal, female, athymic nude mice were used to determine the nanoparticle distribution. The tissue specificity of BN-CLIO-Cy5.5 was determined by comparing the uptake of the nanoparticle in the pancreas and the uptake of ScrBN-CLIO-Cy5.5, a control with similar size and function but different peptide sequence (1). Pancreas injected with BN-CLIO-Cy5.5 had 3-fold higher fluorescence intensity than pancreas injected with Scr-BN-Cy5.5. Both BN-CLIO-Cy5.5 and Scr-BN-Cy5.5 are taken up by Kupffer cells in the liver in a non–receptor-dependent fashion. It appeared that receptor-mediated targeting of BN-CLIO-Cy5.5 occurred in pancreas, whereas high non–peptide-dependent uptake occurred in liver and spleen. The distribution of BN-CLIO-Cy5.5 within the pancreas bearing a tumor was examined ex vivo by fluorescence microscopy. It appeared that the nanoparticle accumulated to the greatest extent at the border of the tumor.

Montet et al. also reported that BN-CLIO-Cy5.5 can improve the MRI contrast in normal pancreas and tumor (1). Pancreatic tumor cell line MIA-PaCa2 was implanted directly in the pancreatic tail of female athymic nude mice 6 days before the image was taken. BN-CLIO-Cy5.5 was introduced through tail-vein injection and images were taken before and 24 h after the administration of the agent. The tumor was barely visible in the precontrast image, but it became clearly identifiable after the darkening of normal pancreas. The T2 values for tumors were 62 ± 6 ms pre-injection and 62 ± 5 ms post-injection. The T2 values for normal pancreas decreased from 46 ± 5 ms pre-injection to 39 ± 5 ms post-injection.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=bombesin%20CLIO%20%28dog%20OR%20sheep%20OR%20rabbit%20OR%20pig%29)]

No relevant publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=bombesin%20CLIO%20%28primate%20NOT%20human%29)]

No relevant publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=bombesin%20CLIO%20human)]

No relevant publication is currently available.

## References

1 Montet X, Weissleder R, Josephson L. (2006). Imaging pancreatic cancer with a Peptide-nanoparticle conjugate targeted to normal pancreas. Bioconjug Chem.
2 Chachuat A Bonnemain B European clinical experience with Endorem. A new contrast agent for liver MRI in 1000 patients Radiologe 1995 35 11Suppl 2S274 S276 8588035
3 Harisinghani MG, Barentsz J, Hahn PF, Deserno WM, Tabatabaei S, van de Kaa CH, de la Rosette J, Weissleder R. (2003). Noninvasive detection of clinically occult lymph-node metastases in prostate cancer. N Engl J Med.
4 Lantry LE, Cappelletti E, Maddalena ME, Fox JS, Feng W, Chen J, Thomas R, Eaton SM, Bogdan NJ, Arunachalam T, Reubi JC, Raju N, Metcalfe EC, Lattuada L, Linder KE, Swenson RE, Tweedle MF, Nunn AD. (2006). 177Lu-AMBA: Synthesis and characterization of a selective 177Lu-labeled GRP-R agonist for systemic radiotherapy of prostate cancer. J Nucl Med.
5 Okarvi SM al-Jammaz I Synthesis, radiolabelling and biological characteristics of a bombesin peptide analog as a tumor imaging agent Anticancer Res 2003 233B2745 2750 12894569
6 Smith CJ, Gali H, Sieckman GL, Hayes DL, Owen NK, Mazuru DG, Volkert WA, Hoffman TJ. (2003). Radiochemical investigations of 177Lu-DOTA-8-Aoc-BBN[7-14]NH2: an in vitro/in vivo assessment of the targeting ability of this new radiopharmaceutical for PC-3 human prostate cancer cells. Nucl Med Biol.
7 Smith CJ Sieckman GL Owen NK Hayes DL Mazuru DG Volkert WA Hoffman TJ Radiochemical investigations of [188Re(H2O)(CO)3-diaminopropionic acid-SSS-bombesin(7-14)NH2]: syntheses, radiolabeling and in vitro/in vivo GRP receptor targeting studies Anticancer Res 2003 231A63 70 12680195
8 Varvarigou AD, Scopinaro F, Leondiadis L, Corleto V, Schillaci O, De Vincentis G, Sourlingas TG, Sekeri-Pataryas KE, Evangelatos GP, Leonti A, Xanthopoulos S, Delle Fave G, Archimandritis SC. (2002). Synthesis, chemical, radiochemical and radiobiological evaluation of a new 99mTc-labelled bombesin-like peptide. Cancer Biother Radiopharm.
9 Fleischmann A, Laderach U, Friess H, Buechler MW, Reubi JC. (2000). Bombesin receptors in distinct tissue compartments of human pancreatic diseases. Lab Invest.
10 Breeman WA, De Jong M, Bernard BF, Kwekkeboom DJ, Srinivasan A, van der Pluijm ME, Hofland LJ, Visser TJ, Krenning EP. (1999). Pre-clinical evaluation of [(111)In-DTPA-Pro(1), Tyr(4)]bombesin, a new radioligand for bombesin-receptor scintigraphy. Int J Cancer.
11 Zachary I, Rozengurt E. (1987). Internalization and degradation of peptides of the bombesin family in Swiss 3T3 cells occurs without ligand-induced receptor down-regulation. EMBO J.
12 Zhu WY, Goke B, Williams JA. (1991). Binding, internalization, and processing of bombesin by rat pancreatic acini. Am J Physiol.
13 Josephson L, Perez JM, Weissleder R. (2001). Magnetic Nanosensors for the Detection of Oligonucleotide Sequences. Angew Chem Int Ed Engl.
14 Josephson L, Tung CH, Moore A, Weissleder R. (1999). High-efficiency intracellular magnetic labeling with novel superparamagnetic-Tat peptide conjugates. Bioconjug Chem.
15 Montet X, Yuan H, Weissleder R, Josephson L. (2006). Enzyme-based visualization of receptor-ligand binding in tissues. Lab Invest.